# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-E(E{E[c(RGDyK)]_2_}_2_)_2_ peptide

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid- E(E{E[c(RGDyK)]_2_}_2_)_2_ peptide
Abbreviated name: | ^64^Cu-DOTA-RGD Octamer
Synonym: | ^64^Cu-Octameric RGD peptide, ^64^Cu-DOTA-E(E{E[c(RGDyK)]_2_}_2_)_2_
Agent Category: | Peptide
Target: | Integrin (Integrin α_v_β_3_)
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal /contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov). Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29)]

^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-E(E{E[c(RGDyK)_2_}_2_)_2_ peptide (^64^Cu-DOTA-RGD octamer) is an integrin-targeted molecular imaging agent developed for positron emission tomography (PET) imaging of tumor vasculature, tumor angiogenesis, and osteoclasts (1). ^64^Cu is a positron emitter with a half-life (t_½_) of 12.7 h.

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiological processes (2, 3). Among the molecules that regulate angiogenesis are integrins, which comprise a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5). These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Expression of integrin α_v_β_3_ receptors on endothelial cells is stimulated by angiogenic factors and environments. The integrin α_v_β_3_ receptor is generally not found in normal tissue but it is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature. Molecular imaging probes carrying the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (6, 7).

Various RGD peptides in both linear and cyclic forms have been developed for in vivo binding to integrin α_v_β_3_ (8). It has been hypothesized that cyclic RGD peptides (RGDfK or RGDyK) may have a faster rate of receptor binding or a slower rate of dissociation from the integrin α_v_β_3_ than linear single-RGD peptides (9). Chen et al. (10) evaluated a cyclic RGD D-Tyr analog peptide [c(RGDyK)] labeled with ^64^Cu or ^18^F in nude mice bearing breast tumors. They used DOTA for c(RGDyK) conjugation with ^64^Cu, and ^64^Cu-DOTA-c(RGDyK) showed prolonged tumor radioactivity retention but persistent liver radioactivity. Wu et al. (9) suggested that a multimeric RGD peptide with more than two repeating cyclic RGD units would further enhance the affinity of the receptor−ligand interactions through the phenomenon of polyvalency. They also suggested that the increase in molecular size might prolong circulation time and reduce tumor washout rate. Consequently, Wu et al. (9) developed a tetrameric RGD D-Phe analog peptide, ^64^Cu-DOTA-E{E[c(RGDfK)_2_}_2_, and they showed that this PET radioligand appeared to have high integrin avidity and favorable biokinetics in nude mice bearing human gliomas. Using the same approach, Li et al. (1) synthesized and evaluated both ^64^Cu-DOTA-RGD tetramer and ^64^Cu-DOTA-RGD octamer.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20synthesis)]

Li et al. (1) reported that ^64^Cu-DOTA-RGD octamer was synthesized through an active ester method by coupling Boc-Glu(OSu)-OSu with E[c(RGDfK)]_2_ followed by deprotection. The monomeric cyclic peptide c(RGDyK) was first prepared via solution cyclization of fully protected linear pentapeptide H-Gly-Asp(OtBu)-D-Tyr(OtBu)-Lys(Boc)-Arg(Pbf)-OH, followed by trifluoroacetic acid (TFA) deprotection in the presence of the free-radical scavenger triisopropylsilane (11). The RGD dimer was then prepared by mixing c(RGDyK) with the Boc-protected glutamic acid–activated ester Boc-Glu(OSu)_2_ in triethylamine and stirring at room temperature overnight (11, 12). This yielded Boc-E[c(RGDyK)]_2_. The Boc-group was then removed by dissolving in anhydrous trifluoroacetic acid (TFA) and stirring at room temperature for 5 min. Similarly, the E(E{E[c(RGDyK)]_2_}_2_)_2_ octamer was prepared by mixing the E{E[c(RGDyK)]_2_}_2_ tetramer with Boc-E(OSu)_2_ at room temperature (pH 8.5−9.0) overnight and removing the Boc-group by treatment with TFA. E(E{E[c(RGDyK)]_2_}_2_)_2_ was purified by high-performance liquid chromatography (HPLC) (9). DOTA-E(E{E[c(RGDyK)]_2_}_2_)_2_ was synthesized by first activating DOTA with 1-ethyl-3-[3-(dimethylamino)propyl]carbodiimide (EDC) and N-hydroxysulfonosuccinimide (SNHS) at pH 5.5 for 30 min to produce DOTA-OSSu, which was then cooled to 4ºC and reacted with E(E{E[c(RGDyK)]_2_}_2_)_2_. The reaction mixture was adjusted to pH 8.5 and incubated overnight. The DOTA-peptide was purified by HPLC with a 67% yield. The identity of DOTA-E(E{E[c(RGDyK)]_2_}_2_)_2_ was confirmed by matrix-assisted laser desorption/ionization time-of-flight mass spectrometry with a molecular weight of 6,122.3 (C_267_H_390_N_83_O_85_; calculated molecular weight = 6,121.9). ^64^Cu-DOTA-E(E{E[c(RGDyK)]_2_}_2_)_2_ was prepared by adding ^64^Cu-chloride in sodium acetate (pH 6.5) to DOTA-E(E{E[c(RGDyK)]_2_}_2_)_2_ and incubated for 1 h at 50ºC. The final radiolabeled peptide was purified by semi-preparative HPLC. The decay-corrected yield of ^64^Cu-DOTA-RGD octamer was 80–90%. The radiochemical purity was >98% and the specific activity was 23 MBq/nmol (0.62 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20in%20vitro)]

Li et al. (1) conducted in vitro cell adhesion assays of unlabeled E(E{E[c(RGDyK)]_2_}_2_)_2_ by using integrin α_v_β_3_−positive human glioblastoma U87MG cells. Fibronectin (non–α_v_β_3_-specific) and vitronectin (α_v_β_3_-specific) were used as competitive ligands. The U87MG cell adhesion ability of fibronectin was not affected by 50–800 nM concentrations of E(E{E[c(RGDyK)]_2_}_2_)_2_. On the other hand, the E(E{E[c(RGDyK)]_2_}_2_)_2_ inhibited vitronectin cell adhesion in a concentration-dependent manner. The receptor-binding affinities of the octamer and DOTA-octamer were studied with the use of ^125^I-echistatin–competitive cell-binding assays (1). The assays showed that the DOTA conjugation had a minimal effect on the receptor-binding avidity. The octamer appeared to have three-fold higher avidity than the tetramer. The inhibition concentration (IC_50_) value (n = 3) calculated for E(E{E[c(RGDyK)]_2_}_2_)_2_ was (1.0 ± 0.2) × 10−^8^ mol/liter. In comparison, the tetrameric E{E[c(RGDyK)]_2_}_2_ and dimeric E[c(RGDyK)]_2_ had IC_50_ values of (3.5 ± 0.3) × 10−^8^ mol/liter and (1.0 ± 0.1) × 10−^7^ mol/liter, respectively. The IC_50_ value for DOTA- E(E{E[c(RGDyK)]_2_}_2_)_2_ was (1.1 ± 0.2) × 10^–8^ mol/liter.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20rodentia)]

Biodistribution studies of ^64^Cu-DOTA-RGD octamer were conducted in normal mice (1). Each mouse received an i.v. dose of 0.74−1.11 MBq (20−30 μCi). At 20 h after injection, the highest radioactivity level was in the kidney, followed by the liver and intestine. The kidney radioactivity level (n = 3) in percent injected dose per g (% ID/g) was 27.0 ± 3.5. The liver and intestine radioactivity levels (extrapolated from Figure 5A) were ~4% ID/g and ~3% ID/g, respectively. The overall clearance was slower than the tetramer. The tetramer had a five-fold lower kidney radioactivity level. With coinjection of 10 mg/kg unlabeled c(RGDyK) as a blocking dose, the radioactivity levels in the kidney and all other major organs were significantly decreased.

MicroPET imaging studies were conducted in nude mice bearing subcutaneous human U87MG gliomas and c-neu mice (which carried an activated c-neu oncogene that spontaneously developed integrin α_v_β_3_-positive mammary adenocarcinomas) (1). Each mouse received ~9.3 MBq (0.25 mCi) ^64^Cu-DOTA-RGD octamer by i.v. administration. The U87MG tumor was clearly visualized with high tumor/background contrast. The radioactivity levels (% ID/g) calculated from quantitative analyses of PET data (n = 3) in the tumors were 11.7 ± 0.7 (0.5 h), 10.6 ± 0.7 (1 h), 10.6 ± 0.3 (2 h), 10.5 ± 0.7 (6 h), and 10.3 ± 1.0 (20 h). The tumor radioactivity washout appeared to be minimal. These tumor radioactivity levels were higher than those of the ^64^Cu-DOTA-RGD tetramer. The coinjected blocking dose of 10 mg/kg c(RDGyK) reduced the tumor radioactivity at 2 h after administration from 10.6 ± 0.3% ID/g to 1.7 ± 0.2% ID/g. The other organ radioactivity levels were similar to the biodistribution pattern in normal mice. The kidney radioactivity level was ~30% ID/g (extrapolated from Figure 4A) at 20 h, and the liver radioactivity was ~3% ID/g at 20 h. In the spontaneous mammary carcinomas, the tumor radioactivity level (n = 3) also reached 8.9 ± 2.1% ID/g at 1 h and decreased to 6.6 ± 1.5% ID/g at 20 h. The radioactivity levels at 20 h in the kidney and liver were ~40% ID/g and ~5% ID/g, respectively (extrapolated from Figure 4B).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIH NIBIB R21 EB001785, NCI CA 102123, P50 CA114747, U54 CA119367, R21CA93862.

## References

1 Li Z.B., Cai W., Cao Q., Chen K., Wu Z., He L., Chen X. (2007). 64Cu-Labeled Tetrameric and Octameric RGD Peptides for Small-Animal PET of Tumor {alpha}v{beta}3 Integrin Expression. J Nucl Med.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Paulhe F., Manenti S., Ysebaert L., Betous R., Sultan P., Racaud-Sultan C. (2005). Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des.
4 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
5 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
6 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
7 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
9 Wu Y., Zhang X., Xiong Z., Cheng Z., Fisher D.R., Liu S., Gambhir S.S., Chen X. (2005). microPET imaging of glioma integrin {alpha}v{beta}3 expression using (64)Cu-labeled tetrameric RGD peptide. J Nucl Med.
10 Chen X., Park R., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). MicroPET and autoradiographic imaging of breast cancer alpha v-integrin expression using 18F- and 64Cu-labeled RGD peptide. Bioconjug Chem.
11 Chen X., Park R., Shahinian A.H., Bading J.R., Conti P.S. (2004). Pharmacokinetics and tumor retention of 125I-labeled RGD peptide are improved by PEGylation. Nucl Med Biol.
12 Liu S., Hsieh W.Y., Kim Y.S., Mohammed S.I. (2005). Effect of coligands on biodistribution characteristics of ternary ligand 99mTc complexes of a HYNIC-conjugated cyclic RGDfK dimer. Bioconjug Chem.